# Perflexane-Lipid Microspheres

Chemical name: | Perflexane-Lipid Microspheres
Abbreviated name: | AFO150
Synonym: | Imagent®, Imavist®, n-perfluorohexane emulsion, AFO145
Agent Category: | Lipid microspheres
Target: | Non-targeted agent, cardiac chambers
Target Category: | Passive nonspecific filling of cardiac chambers
Method of detection: | Ultrasound (US)
Source of signal/contrast: | Microbubbles and perflexane gas
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Humans | Click on the above structure of perflexane for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Imagent%20or%20perflexane%20or%20AFO150%20or%20Imavist)]

Perflexane-lipid microspheres (AFO150) is a preparation of perfluorocarbon (PFC)-based microbubbles that was developed as an ultrasound (US) contrast agent for use in echocardiograms to enhance US images (1-3). In the United States, it was approved by the Food and Drug Administration in 2002 for clinical use in echocardiograms to opacify the left ventricular chamber and to improve the delineation of the left ventricular endocardial border. However, AFO150 is not currently available for clinical applications.

US contrast agents or echopharmaceuticals are designed to change the attenuation (absorption, reflection, and refraction) or impedance (resistance to sound propagation) of sound for enhancing the differentiation of the signal (echo) of a target organ from that of the surrounding tissue (3-6). Gas-liquid emulsions (microbubbles or gaseous particles) are highly echogenic invivo because of the nonlinear rarefaction and compression effects that lead to volume pulsations of microbubbles (3, 7, 8). Human serum albumin, synthetic polymers and phospholipids have been used to construct the membrane of these bubbles. Microbubble preparations of various formulations have been developed, and their clinical usefulness depends very much on the size and stability of these bubbles in vivo.

PFCs are inert, volatile chemicals and can be encapsulated within the microbubbles to provide a stabilizing effect. The extremely low water solubility of PFCs sets up an equilibrium in vivo where the water-soluble gases diffuse in and out of the microbubble, but the PFC vapor counterbalances the surface tension and blood pressure forces that push the gases inside the bubble toward dissolution. As a result, the combined properties of the microbubble shell and the PFC gas inside determine the stability and output signal of each microbubble in vivo. PFC emulsions were initially studied as oxygen carriers (blood substitutes) (9, 10). Perfluorooctyl bromide (C_8_BrF_17_), a compound similar to perflexane (C_6_F_14_), was first discovered to possess sufficient lipophilicity to be formulated into stable emulsions but was developed as an oral agent for negative magnetic resonance imaging of the gastrointestinal tract (11).

AFO150 was developed based on the concept of osmotic stabilization of the microbubbles by a mixture of nitrogen gas and perflexane (1-3). The preparation formulation uses a semi-synthetic phospholipid, dimyristoylphosphatidylcholine (DMPC), for forming the lipid microsphere shell and hydroxyethyl starch to serve as a mold or template for the desired bubbles. The commercial product contains a powder of 200 mg of spray-dried, micrometer-sized hollow and porous spheres under a gas mixture of nitrogen and perflexane. Upon reconstitution with sterile water (5.9-13.7 × 10^8^ microspheres/ml) and i.v. administration to a patient, the preparation produces approximately 3-µm microbubbles with a single layer of phospholipid membrane that encloses the perflexane/nitrogen gases within the targeted organ.

Serious cardiopulmonary reactions following the administration of ultrasound microbubble contrast agents have been reported (12). In 2007, the US FDA (http://www.fda.gov/cder/drug/InfoSheets/HCP/microbubbleHCP.htm) requested that warnings emphasizing the risk for serious cardiopulmonary reactions be added to the labeling of these agents. The uses of these agents are contraindicated in patients with unstable cardiopulmonary status.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Imagent%20or%20perflexane%20or%20Imavist%20or%20perflubron%29%20AND%20synthesis)]

PFCs are inert organic materials initially developed for handling the extremely corrosive uranium fluorides (9, 10, 13). Some PFCs are directly derived from the manufacturing line that led to Teflon and other diverse industrial surfactants. Two major strategies are commonly used in producing PFCs. One strategy is substituting fluorine atoms for hydrogen atoms in the parent hydrocarbon analog by electrochemical fluorination, fluorination by high-valency metal fluorides, or direct fluorination. Another strategy is combining smaller, reactive fluorinated building blocks by telomerization.

Natural egg yolk and synthetic phospholipids have been used to produce the microbubbles in the emulsion preparation. The commercial preparation of AFO150 uses DMPC to form the microspheres. Harbison and Griffin (14) reported a high-yield (76%) synthesis method of DMPC with the use of dimyristoylphosphatidic acid.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Imagent%20or%20Imavist%20or%20perflexane%29%20AND%20in%20vitro)]

In an in vitro study using normal saline solution bags in a water tank, a direct relationship between the US energy and microbubble destruction was found in perflexane-lipid microspheres and two other US contrast agents (15). Another study found that the US energy-mediated destruction of microbubbles was a function of US intensity, duration, and frequency (16). In a flow model in which the AFO150 microbubbles flowed through a gelatin matrix, the relative intensity threshold for bubble destruction was 1-5 watts/cm^2^ (2). In vitro genetic toxicity studies of AFO150 (bacterial reverse mutation assay, chromosomal aberration assay, and forward mutation assay with mouse lymphoma cells) were reported to be negative (17).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28imagent%20or%20imavist%20or%20perflexane%29%20AND%20rodentia)]

The impact of myocardial contrast echocardiography (MCE) on vascular permeability caused by AFO150 and two other agents (perflutren-lipid microspheres and perflutren protein-type A microspheres) was studied with US imaging at 1.7 MHz in rats (18). All three agents appeared to have equal potential of inducing microvascular leakage when compared on the basis of relatively high microbubble doses (25-200 µl/kg for AFO150) (18). Mattrey et al. (19) studied possible placental perfusion assessment with perflexane-lipid microspheres (0.1-0.3 ml) at 7 MHz in pregnant rats, and they found marked US image enhancement of the rat placenta that showed the potential of using the agent for maternal placental imaging.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Imavist%20or%20imagent%20or%20perflexane%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

An imaging study of the effect of US intensity on contrast appearance of perflexane-lipid microspheres (0.015-0.03 ml/kg) and two other US agents was conducted in mongrel dogs (n=3) (15). All three preparations of microbubbles were found to be destroyed or substiantially modified within the ventricle by high US transmit powers at 5 MHz with the attenuation changed from 0 dB to more than -6 dB (up to -9 dB).

Using radioactive microsphere technology to measure myocardium perfusion in dogs (n=18) with varying coronary stenosis severity, Wei and colleagues (20) reported that both bolus injection and continuous infusion of AFO150 in MCE (transmitted at 2 MHz) provided quantitative assessment of relative coronary stenosis severity. Another study also reported that MCE (transmitted at 1.67 MHz) with the use of AFO150 accurately detected the dynamic changes in blood flow during reperfusion in mongrel dogs (n=16) with coronary occlusion (21). Other studies in rabbits and dogs have shown potential applications of AFO150 for enhancing US imaging of the liver, kidneys, CNS, and lymph nodes [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Imavist%20or%20imagent%20or%20perflexane%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)].

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28imavist%20OR%20imagent%20OR%20perflexane%20OR%20perflubron%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28imavist%20or%20imagent%20or%20perflexane%29%20AND%20human)]

In healthy volunteers (n=12), a single i.v. dose (4 mg/kg) of AFO150 showed clearance in a multi-exponential fashion with mean elimination half-lives in blood and expired air of approximately 5.3 ± 6.1 h and 9.0 ± 5.0 h, respectively (1, 2, 22). Females appeared to eliminate perflexane through expired air more slowly than males.

In the Phase I trial of a single-blind, dose-ranging (0.125-4.0 mg/kg) study of 44 normal volunteers, minor adverse events (headache, nausea, and dizziness) were reported for 3 subjects (23). US imaging revealed marked gray-scale contrast enhancement of the left ventricle and opacification of the myocardium at all doses in all subjects.

Two clinical studies of a total of 409 patients who received a single i.v. bolus of 0.125 mg/kg of AFO150 were performed with two-dimensional MCE and evaluated by three blinded, independent readers (1, 2, 22, 24). The results showed statistically significant (P<0.0001) improvement in total endocardial border delineation scores (changes ranged from a mean of 4.9 to 10.5) when MCE with the use of AFO150 was compared with non-contrast baseline imaging.

## Supplemental Information

[Disclaimers]

FDAImagent

Imagentpackageinsert

## NIH Support

US Public Health Service EB00338, NHLBI R01-HL48890, F32-HL095410.

## References

1 (2002). AFO 150, Imagent, Imavist). Drugs R D.
2 (2002). AFO 150. Imagent, Imavist. Drugs R D.
3 Schutt E.G., Klein D.H., Mattrey R.M., Riess J.G. (2003). Injectable microbubbles as contrast agents for diagnostic ultrasound imaging: the key role of perfluorochemicals. Angew Chem Int Ed Engl.
4 Morawski A.M., Lanza G.A., Wickline S.A. (2005). Targeted contrast agents for magnetic resonance imaging and ultrasound. Curr Opin Biotechnol.
5. Swanson, D.P., Enhancement agents for ultrasound: Fundamentals, in Pharmaceuticals in Medical Imaging, D.P. Swanson, H.M. Chilton and J.H. Thrall, Editor. 1990, MacMillan Publishing Co., Inc.: New York. p. 682-687.
6. Gobuty, A.H., Perspectives in ultrasound contrast agents, in Contrast media: Biologic effects and clinical application, Z. Parvez, R. Moncada and M. Sovak, Editor. 1987, CRC: Boca Raton, Florida. p. 145-155.
7 Averkiou M., Powers J., Skyba D., Bruce M., Jensen S. (2003). Ultrasound contrast imaging research. Ultrasound Q.
8 Miller A.P., Nanda N.C. (2004). Contrast echocardiography: new agents. Ultrasound Med Biol.
9 Riess J.G. (2001). Oxygen carriers ("blood substitutes")--raison d'etre, chemistry, and some physiology. Chem Rev.
10 Riess J.G. (2002). Blood substitutes and other potential biomedical applications of fluorinated colloids. Journal of Fluorine Chemistry.
11 Mattrey R.F., Trambert M.A., Brown J.J., Bruneton J.N., Young S.W., Schooley G.L. (1991). Results of the phase III trials with Imagent GI as an oral magnetic resonance contrast agent. Invest Radiol.
12 Blomley M., Claudon M., Cosgrove D. (2007). WFUMB Safety Symposium on Ultrasound Contrast Agents: clinical applications and safety concerns. Ultrasound Med Biol.
13 Riess J.G. (2002). Fluorous micro- and nanophases with a biochemical perspective. Tetrahedron.
14 Harbison G.S., Griffin R.G. (1984). Improved method for the synthesis of phosphatidylcholines. J Lipid Res.
15 Villarraga H.R., Foley D.A., Aeschbacher B.C., Klarich K.W., Mulvagh S.L. (1997). Destruction of contrast microbubbles during ultrasound imaging at conventional power output. J Am Soc Echocardiogr.
16 Walker K.W., Pantely G.A., Sahn D.J. (1997). Ultrasound-mediated destruction of contrast agents. Effect of ultrasound intensity, exposure, and frequency. Invest Radiol.
17 Alliance Pharmaceuticals I. (2002). Imagent Package Insert. Kit for he preparation of perflexane lipid microspheres injectable suspension for intravenous administration.. p. 4-18.
18 Li P., Armstrong W.F., Miller D.L. (2004). Impact of myocardial contrast echocardiography on vascular permeability: comparison of three different contrast agents. Ultrasound Med Biol.
19 Mattrey R.F., Baker K.G., Hall L.A., Steinbach G.C., Peterson T. (1996). Placental enhancement with AF0145, a perfluorocarbon-stabilized microbubble sonographic contrast agent. Acad Radiol.
20 Wei K., Jayaweera A.R., Firoozan S., Linka A., Skyba D.M., Kaul S. (1998). Basis for detection of stenosis using venous administration of microbubbles during myocardial contrast echocardiography: bolus or continuous infusion?. J Am Coll Cardiol.
21 Galiuto L., DeMaria A.N., May-Newman K., Del Balzo U., Ohmori K., Bhargava V., Flaim S.F., Iliceto S. (1998). Evaluation of dynamic changes in microvascular flow during ischemia-reperfusion by myocardial contrast echocardiography. J Am Coll Cardiol.
22 (2002). . Kit for he preparation of perflexane lipid microspheres injectable suspension for intravenous administration. Alliance Pharmaceuticals, Inc., : p. 4-18.
23 Pelura T.J. (1998). Clinical experience with AF0150 (Imagent US), a new ultrasound contrast agent. Acad Radiol.
24 Nanda N.C., Kitzman D.W., Dittrich H.C., Hall G. (2003). Imagent improves endocardial border delineation, inter-reader agreement, and the accuracy of segmental wall motion assessment. Echocardiography.